# [^125^I]N-(4-Dipropylaminobutyl)-4-iodobenzamide

Chemical name: | [^125^I]N-(4-Dipropylaminobutyl)-4-iodobenzamide
Abbreviated name: | [^125^I]BZ18
Synonym:
Agent Category: | Compounds
Target: | Melanin
Target Category: | Others
Method of detection: | Single-photon emission computed tomography (SPECT), planar imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Chemical structure is not available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=benzamide+and+imaging+and+therapy)]

Radioiodinated N-(4-dipropylaminobutyl)-4-iodobenzamide, abbreviated as [^125^I]BZ18, is a benzamide (BZA) derivative that was synthesized for melanin-targeted radionuclide imaging and therapy of melanoma (1, 2).

BZA derivatives represent a versatile class of aromatic compounds that possess a common structure element of Ph-CONH(CH_2_)_m_NR_2_ (m = 1, 2) and exhibit comparable properties, including high and specific binding with melanin in melanoma cells and melanocytes (3-5). Some of these compounds, such as N-(2-diethylaminoethyl)-4-[^123^I]iodobenzamide ([^123^I]BZA) and [^123^I]-N-(2-diethylaminoethyl)-2-iodobenzamide ([^123^I]BZA2), have been successfully evaluated in melanoma patients, showing high sensitivity and selectivity in the detection of melanoma and its metastasis (6-9).

The promising results with [^123^I]BZA have prompted great efforts from several groups in screening BZA analogs (2, 3, 10). Among them is a group of investigators in France who synthesized a series of BZA derivatives via structure-activity studies (1, 6, 11, 12). On the basis of the structure of the lead agent [^123^I]BZA, they synthesized a group of spermidine BZA derivatives by replacing the diethylaminoethyl moiety in the BZA structure with a triamine (spermidine). Spermidine BZA derivatives exhibit high affinity for melanin comparable to that of [^123^I]BZA; however, these compounds exhibit less accumulation in tumors than [^123^I]BZA in animal models of melanoma (13). More recently, the investigators generated a class of heteroaromatic BZA analogs by incorporating the heteroaromatic structure in place of the benzene moiety to take advantage of the polycyclic aromatic compounds that display a strong affinity for melanin while keeping the lipophilic side chain (14). The heteroaromatic analogs, [^125^I]5a through [^125^I]5I, showed high specific and long-lasting uptake in the melanoma, which is favorable for both imaging and therapy (14). At the same time, the investigators also identified a group of quinoxaline analogs; the radioiodinated derivative 3 (ICF01012) is one of these compounds, which show the most favorable pharmacokinetic properties for radionuclide therapy (12, 15). The rapid and specific tumor uptake of quinoxaline compounds also suggests that they are potentially valuable for radionuclide imaging. For radiofluorination, ICF01012 was modified by incorporating 2- or 6-fluoropyridine in the N,N-diethylethylenediamine framework of ICF01012 (16). This strategy allows nucleophilic heteroaromatic radiofluorination of corresponding halogeno- or nitro-precursors without the need for an additional electron-withdrawing substituent in the aromatic ring. Fluoropyridine was introduced on the tertiary amine either directly or in combination with various linkers, which resulted in a group of amide tracers, such as the agents [^125^I]56 and [^18^F]44 (compound 56 is the dihydrochloride salt of 44) (16). These derivatives showed favorable properties for combined radionuclide imaging (^18^F, ^125^I) and therapy (^131^I) of melanoma using a single chemical structure. The following is a list of some representative agents that were synthesized and tested by the investigators from the group in France.

BZA derivatives: [^125/123^I]BZA, [^125^I]BZA2, [^125^I]BZ18, and [^125^I]5a through [^125^I]5l; and quinoxaline derivatives: [^125/131^I]ICF01012 (or [^125/131^I]3), [^125^I]56, and [^18^F]44.

This chapter summarizes the data of imaging studies obtained with [^125^I]BZ18 (1, 2).

### Related Resource Links:

Melanin-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=melanin+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Benzamide derivatives in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?db=pcsubstance&term=benzamide) Benzamide derivatives in clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=benzamide)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Moins,+N)]

BZ18 was synthesized by the reaction of 4-diethylaminobutylamine and 4-iodobenzoyl chloride (1, 2). Labarre et al. labeled BZ18 by electrophilic radio-iododestannylation of the tributyl stannyl precursor using no-carrier-added [^125^I]NaI. From different synthetic batches of [^125^I]BZ18, the yields of iodination were in the range of 50%–60%, with a radiochemical purity of >99% and a high specific activity of 180 GBq/mg (4.86 Ci/mg) (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Moins,+N)]

Binding of [^125^I]BZ18 to melanin was measured after incubation of [^125^I]BZ18 with synthetic tyrosine-melanin in water (1). Scatchard plot analysis indicated two classes of binding sites, one with a high association constant (K_1_ = 5.7 × 10^7^ M−^1^), and a second one with a lower association constant (K_2_ = 4.2 × 10^5^ M−^1^).

Radiotoxicity was studied with a method of B16F0 clonogenic survival in different conditions of exposure (1). Results showed that the unlabeled BZ18 (2 × 10−^5^ M) was not cytotoxic. On the contrary, [^125^I]BZ18 induced cytotoxicity that was radioactivity-dependent, and the toxic effect was complete with 2.2 MBq (0.059 mCi) per well. The cytotoxicity was also dependent on incubation time for a given radioactive concentration (data not shown).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Moins,+N)]

Labarre et al. investigated the biodistribution of [^125^I]BZ18 in mouse (1). Whether the animals were pretreated with Lugol’s iodine solution to block thyroid uptake was not reported.

In male C57Bl6 mice bearing B16F0 murine melanoma (n = 3 mice), the tumor uptake of [^125^I]BZ18 after injection of 0.37 MBq/10−^7^ mol (0.01 mCi/10−^7^ mol) was ~10% injected dose per gram of tissue (ID/g) between 1 h and 3 h, and remained at 3.2% ID/g at 72 h after injection. Low radioactive levels were observed in blood, muscle, and brain. [^125^I]BZ18 was washed out from almost all of the organs except for tumor and uvea at 6 h after injection, giving high tumor/nontarget organ ratios.

The effect of [^125^I]BZ18 concentration on its biodistribution was assessed with a fixed dose of 0.37 MBq (0.01 mCi) [^125^I]BZ18 but at different concentrations ranging from 10−^11^ to 10−^6^ mol per mouse (n = 30 mice). The radioactivity in the melanoma and uvea did not differ for each time point at any of the doses studied. However, the radioactivity in the liver increased with increased concentration at 3 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Moins,+N)]

Labarre et al. also investigated the biodistribution of [^125^I]BZ18 in sheep models of melanoma (1). Whether the animals were pretreated with Lugol’s iodine solution to block thyroid uptake was not reported.

The sheep models of tumors were generated by inoculating the cells of murine B16F0, human SK amelanotic melanoma, Malme melanotic melanoma, and LS174T human colonic carcinoma at different sites (n = 11 sheep). Sheep were euthanized at different time points. After injection of 14 MBq (0.38 mCi) [^125^I]BZ18, radioactivity was detected in all tumors and organs examined from day 1 to day 3. On day 6 after injection, radioactivity in SK melanoma and LS174T colonic carcinoma became undetectable. On days 9 and 12 after injection, only blood, Malme melanoma, B16 melanoma, lymph nodes, and uveal tract showed detectable radioactivity. In more detail, a high uptake in B16 melanoma (0.0214% ID/g) was observed on day 1, and the uptake was maintained for a long time (0.0086% ID/g on day 12). The uptake in both SK melanoma and LS174T colonic carcinoma was very low (<0.0006% ID/g on day 1 and <0.00009% ID/g on day 3 after injection). For the Malme melanoma, the uptake was moderate on day 1 (0.004% ID/g) and low from day 3 after injection. Fast clearance of the radioactivity from normal tissues was observed except in the uveal tract (0.063% ID/g on day 1 and 0.027% ID/g on day 12). There was no radioactivity in the thyroid.

The kinetic uptake of [^125^I]BZ18 in three sheep bearing only B16 melanoma was assessed from 1 h to 48 h after injection. The uptake in B16 melanoma reached a plateau at 1 h after injection. Respective concentrations in blood were low. The tumor/blood ratios were in the range of 14.8–558 from 1 h to 48 h after injection.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Labarre P., Papon J., Rose A.H., Guerquin-Kern J.L., Morandeau L., Wu T.D., Moreau M.F., Bayle M., Chezal J.M., Croisy A., Madelmont J.C., Turner H., Moins N. (2008). Melanoma affinity in mice and immunosuppressed sheep of [(125)I]N-(4-dipropylaminobutyl)-4-iodobenzamide, a new targeting agent. Nucl Med Biol.
2 Moins N., Papon J., Seguin H., Gardette D., Moreau M.F., Labarre P., Bayle M., Michelot J., Gramain J.C., Madelmont J.C., Veyre A. (2001). Synthesis, characterization and comparative biodistribution study of a new series of p-iodine-125 benzamides as potential melanoma imaging agents. Nucl Med Biol.
3 Oltmanns D., Eisenhut M., Mier W., Haberkorn U. (2009). Benzamides as melanotropic carriers for radioisotopes, metals, cytotoxic agents and as enzyme inhibitors. Curr Med Chem.
4 Chehade F., De Labriolle-Vaylet C., Michelot J., Moins N., Moreau M.F., Hindie E., Papon J., Escaig F., Galle P., Veyre A. (2001). Distribution of I-BZA (N-2-diethylaminoethyl-4-iodobenzamide) in grafted melanoma and normal skin: a study by secondary ion mass spectroscopy. Cell Mol Biol (Noisy-le-grand).
5 Greguric I., Taylor S.R., Denoyer D., Ballantyne P., Berghofer P., Roselt P., Pham T.Q., Mattner F., Bourdier T., Neels O.C., Dorow D.S., Loc'h C., Hicks R.J., Katsifis A. (2009). Discovery of [18F]N-(2-(diethylamino)ethyl)-6-fluoronicotinamide: a melanoma positron emission tomography imaging radiotracer with high tumor to body contrast ratio and rapid renal clearance. J Med Chem.
6 Bacin F., Michelot J., Bonafous J., Veyre A., Moreau M.F., Kemeny J.L., Chossat F., Bekhechi D. (1998). Clinical study of [123I] N-(2-diethylaminoethyl)-4-iodobenzamide in the diagnosis of primary and metastatic ocular melanoma. Acta Ophthalmol Scand.
7 Michelot J.M., Moreau M.F., Veyre A.J., Bonafous J.F., Bacin F.J., Madelmont J.C., Bussiere F., Souteyrand P.A., Mauclaire L.P., Chossat F.M., et al. (1993). Phase II scintigraphic clinical trial of malignant melanoma and metastases with iodine-123-N-(2-diethylaminoethyl 4-iodobenzamide). J Nucl Med.
8 Mansard S., Papon J., Moreau M.F., Miot-Noirault E., Labarre P., Bayle M., Veyre A., Madelmont J.C., Moins N. (2005). Uptake in melanoma cells of N-(2-diethylaminoethyl)-2-iodobenzamide (BZA2), an imaging agent for melanoma staging: relation to pigmentation. Nucl Med Biol.
9 Moins N., D'Incan M., Bonafous J., Bacin F., Labarre P., Moreau M.F., Mestas D., Noirault E., Chossat F., Berthommier E., Papon J., Bayle M., Souteyrand P., Madelmont J.C., Veyre A. (2002). 123I-N-(2-diethylaminoethyl)-2-iodobenzamide: a potential imaging agent for cutaneous melanoma staging. Eur J Nucl Med Mol Imaging.
10 Labarre P., Papon J., Moreau M.F., Moins N., Bayle M., Veyre A., Madelmont J.C. (2002). Melanin affinity of N-(2-diethylaminoethyl)-4-iodobenzamide, an effective melanoma imaging agent. Melanoma Res.
11 Desbois N., Gardette M., Papon J., Labarre P., Maisonial A., Auzeloux P., Lartigue C., Bouchon B., Debiton E., Blache Y., Chavignon O., Teulade J.C., Maublant J., Madelmont J.C., Moins N., Chezal J.M. (2008). Design, synthesis and preliminary biological evaluation of acridine compounds as potential agents for a combined targeted chemo-radionuclide therapy approach to melanoma. Bioorg Med Chem.
12 Bonnet M., Mishellany F., Papon J., Cayre A., Penault-Llorca F., Madelmont J.C., Miot-Noirault E., Chezal J.M., Moins N. (2010). Anti-melanoma efficacy of internal radionuclide therapy in relation to melanin target distribution. Pigment Cell Melanoma Res.
13 Moreau M.F., Papon J., Labarre P., Moins N., Borel M., Bayle M., Bouchon B., Madelmont J.C. (2005). Synthesis, in vitro binding and biodistribution in B16 melanoma-bearing mice of new iodine-125 spermidine benzamide derivatives. Nucl Med Biol.
14 Chezal J.M., Papon J., Labarre P., Lartigue C., Galmier M.J., Decombat C., Chavignon O., Maublant J., Teulade J.C., Madelmont J.C., Moins N. (2008). Evaluation of radiolabeled (hetero)aromatic analogues of N-(2-diethylaminoethyl)-4-iodobenzamide for imaging and targeted radionuclide therapy of melanoma. J Med Chem.
15 Bonnet-Duquennoy M., Papon J., Mishellany F., Labarre P., Guerquin-Kern J.L., Wu T.D., Gardette M., Maublant J., Penault-Llorca F., Miot-Noirault E., Cayre A., Madelmont J.C., Chezal J.M., Moins N. (2009). Targeted radionuclide therapy of melanoma: anti-tumoural efficacy studies of a new 131I labelled potential agent. Int J Cancer.
16 Maisonial A., Kuhnast B., Papon J., Boisgard R., Bayle M., Vidal A., Auzeloux P., Rbah L., Bonnet-Duquennoy M., Miot-Noirault E., Galmier M.J., Borel M., Askienazy S., Dolle F., Tavitian B., Madelmont J.C., Moins N., Chezal J.M. (2011). Single photon emission computed tomography/positron emission tomography imaging and targeted radionuclide therapy of melanoma: new multimodal fluorinated and iodinated radiotracers. J Med Chem.